# [^11^C]Glycylsarcosine

Chemical name: | [^11^C]Glycylsarcosine
Abbreviated name: | [^11^C]Gly-Sar
Synonym:
Agent category: | Peptide
Target: | H^+^/peptide transporters (PEPTs)
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gly-Sar)]

H^+^/Peptide transporters (PEPTs) are members of the proton-coupled peptide transporter SLC15A family (1). PEPT1 is present in the epithelial cells of the small intestine, kidney, and bile duct, whereas PEPT2 is present in the epithelial cells of the kidney, lung, mammary gland, and choroid plexus, as well as in glial cells in the brain (2, 3). PEPTs transport various peptides and peptide-mimetics. PEPT1 is overexpressed in some cancer cells. PEPT1 is expressed in the human fibrosarcoma HT1080 cell line but not in the normal fibroblast IMR-90 cell line (4). [^11^C]Glycylsarcosine ([^11^C]Gly-Sar) has been developed as a positron emission tomography (PET) tracer for imaging PEPTs in cancer cells (5, 6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Gly-Sar+and+synthesis)]

Nabulsi et al. (6) synthesized [^11^C]Gly-Sar in two steps. First, ^11^C-methylation of glycylglycine ethyl ester with [^11^C]methyl triflate was performed for 1 min at 170ºC. A mixture of triethylamine and ammonium acetate was added to the reaction vial and heated for 5 min at 80°C to form [^11^C]cyclo(Gly-Sar), which was purified with high-performance liquid chromatography. The radiochemical yield (decay-corrected) was 5.9% with >99% radiochemical purity. Second, [^11^C]cyclo(Gly-Sar) was hydrolyzed with 2 N NaOH for 8 min at 100°C to form [^11^C]Gly-Sar with a specific activity of 51.8 GBq/µmol (1.4 Ci/µmol), a radiochemical purity of >99%, and a radiochemical yield of 8.6% (decay-corrected, n = 8). The total synthesis time was 42 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Gly-Sar+and+in+vitro)]

In vitro uptake studies were performed using AsPC-1, MKN45, and PC-3 cancer cell lines with 2 µM [^3^H]Gly-Sar (5). The initial uptake rates were 3.88, 1.64, and 1.39 µL/min per mg protein, respectively. The presence of 20 mM Gly-Sar inhibited the uptake rates to 0.94, 0.77, and 1.22 µL/min per mg protein, respectively. The uptake of [^3^H]Gly-Sar by these three cell lines correlated with their PEPT1 mRNA expression (AsPC-1 > MKN45 > PC-3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Gly-Sar+and+rodentia)]

Nabulsi et al. (6) reported biodistribution studies of [^11^C]Gly-Sar in normal mice (n = 4 mice/group). The mice showed high accumulation of radioactivity in the kidneys (~14% injected dose (ID)/g), followed by the spleen (~7% ID/g), lung (~3% ID/g), and liver (~2% ID/g) at 10 min after injectionthe pancreas was not studied) little accumulation was observed in the brain. Whole-body PET imaging confirmed the high accumulation in the kidney medulla. Mitsuoka et al. (5) performed biodistribution studies in nude mice bearing AsPC-1, MKN45, or PC-3 tumor xenografts. Tumor accumulation was rapid and reached a plateau 5–60 min after injection. The standard uptake values at 60 min were 0.70, 0.42, and 0.53, whereas the tumor/muscle ratios at 30 min were 5.0, 2.8, and 3.5 for AsPC-1, MKN45, and PC-3, respectively. High accumulation was found in the kidneys, followed by the pancreas, lung, and liver (the spleen was not studied). Whole-body PET imaging revealed high radioactivity in the kidneys and urinary bladder. All three tumors were clearly visualized. In another study, whole-body PET imaging was performed in nude mice bearing the AsPC-1 tumor xenografts and turpentine-induced inflammation in the opposite hind legs. [^18^F]FDG was also used to compare with [^11^C]Gly-Sar. The tumor/blood ratio (4.0) of [^11^C]Gly-Sar was greater than the muscle/blood (1.7) and inflammation/blood (1.4) ratios. The inflammation/blood ratio (5.8) of [^18^F]FDG was greater than the muscle/blood (1.3) and tumor/blood (4.0) ratios. The selectivity index (tumor/inflammation ratio corrected for normal muscle) was 25.1 for [^11^C]Gly-Sar and 0.72 for [^18^F]FDG. Immunohistochemistry of PEPT1 and PEPT2 studies confirmed the presence of PEPTs in all three tumor xenografts and kidneys, whereas inflammatory tissues and normal muscle were marginal for PEPTs. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Gly-Sar+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Gly-Sar+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Gly-Sar+and+human)]

No publication is currently available.

## Human Studies

CA009015, R01 GM035498

## References

1 Herrera-Ruiz D., Knipp G.T. (2003). Current perspectives on established and putative mammalian oligopeptide transporters. J Pharm Sci.
2 Groneberg D.A., Fischer A., Chung K.F., Daniel H. (2004). Molecular mechanisms of pulmonary peptidomimetic drug and peptide transport. Am J Respir Cell Mol Biol.
3 Rubio-Aliaga I., Daniel H. (2002). Mammalian peptide transporters as targets for drug delivery. Trends Pharmacol Sci.
4 Nakanishi T., Tamai I., Sai Y., Sasaki T., Tsuji A. (1997). Carrier-mediated transport of oligopeptides in the human fibrosarcoma cell line HT1080. Cancer Res.
5 Mitsuoka K., Miyoshi S., Kato Y., Murakami Y., Utsumi R., Kubo Y., Noda A., Nakamura Y., Nishimura S., Tsuji A. (2008). Cancer detection using a PET tracer, 11C-glycylsarcosine, targeted to H+/peptide transporter. J Nucl Med.
6 Nabulsi N.B., Smith D.E., Kilbourn M.R. (2005). [11C]Glycylsarcosine: synthesis and in vivo evaluation as a PET tracer of PepT2 transporter function in kidney of PepT2 null and wild-type mice. Bioorg Med Chem.